# 4,5-Diethyl-10,23-dimethyl-9,24-bis(3-hydroxypropyl)-16,-17-bis(3,hydroxypropyl)oxy-13,20,25,26,27—pentaazapentacyclo-[20.2.1.1^3,6^.1^9,11^.0^14,19^]heptacosa-3,5,8,10,12,14,16,18,20,22,24-undecaene gadolinium hydrates

Chemical name: | 4,5-Diethyl-10,23-dimethyl-9,24-bis(3-hydroxypropyl)-16,-17-bis(3,hydroxypropyl)oxy-13,20,25,26,27—pentaazapentacyclo-[20.2.1.1^3,6^.1^9,11^.0^14,19^]heptacosa-3,5,8,10,12,14,16,18,20,22,24-undecaene gadolinium hydrates
Abbreviated name: | MGd
Synonym: | Motexafin gadolinium, Gadolinium texaphyrin, Xcytrin, Gd-Tex, PCI-0120, Gd texaphyrin, GdT2B2
Agent category: | Small molecule
Target: | Other
Target category: | Other
Method of detection: | Magnetic Resonance Imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Motexafin gadolinium))]

Porphyrins are well known to be selectively localized in tumors, although the mechanism is not completely understood (1). Certain metalloporphyrins have demonstrated a high affinity for a variety of tumor types including carcinoma, sarcoma, neuroblastoma, and melanoma (2, 3). Combined with the ability to enhance relaxation rates of water protons, metalloporphyrins containing paramagnetic metals like Mn(II) exhibit significant efficacy for the detection, delineation, and staging of tumors in magnetic resonance imaging (MRI) (2, 4). Compared with the use of labeled antibodies for tumor-specific imaging, this approach is not limited by antibody specificity and has high tumor uptake and low cost per dose (2). Gadolinium (Gd) as a lanthanide cation can provide higher efficacy to enhance contrast than manganese because it has seven unpaired electrons instead of five (5). However, porphyrin-related tetrapyrrole macrocycles are inadequate to accommodate large cations like lanthanides (6). Thus, an unprecedented porphyrin-like aromatic ligand named texaphyrin has been synthesized by expanding the macrocycle of porphyrins (7). This novel macrocycle has a pentadentate binding core in a near-circular structure with ~20% larger capacity compared to the tetrapyrrolic analogs of porphyrins (7, 8).

Texaphyrin Gd is a highly stable complex widely known as motexafin Gd (abbreviated as MGd) (9). The Gd(III) cation in the complex is coordinated to all five core nitrogen atoms in a 1:1 fashion and leaves four coordinated sites for the structural water molecules in the inner shell (7). The T_1_ relaxivity is approximately three to four times greater than that of conventional contrast agents such as gadolinium-diethylenetriamine pentaacetic acid (Gd-DTPA) (10). The open architecture and large number of side chains also provide ample opportunity to outer sphere interactions by hydrogen bonding to the ligand or by close translation of water molecules (10). Unlike many metalloporphyrins, MGd is not a photosensitizer because the strong paramagnetism of the Gd(III) cation promotes efficient relaxation of the excited electronic state (10, 11). The lipophilicity and hydrophilicity in the ligand texaphyrin can be manipulated to enhance the efficacy of selective tissue targeting (10).

MGd has multiple potential applications in cancer treatments in addition to its use in MRI, such as being a single therapeutic agent, either in conjunction with other anticancer agents or concomitantly with radiation therapy (9). This arises from the fact that the ligand can formulate as an 18 π-electron annulene or as an overall 22 π-electron system (8). Therefore, MGd has a high electron affinity and is easily reduced (half-wave potential -0.041 mV versus normal hydrogen electrode) (9, 11). In vivo, MGd is a redox mediator that catalyzes slow oxidation of intracellular reducing metabolites such as ascorbates, glutathione, dihydrolipoate, nicotinamide adenine dinucleotide phosphate (NADP), and protein thiols and generates superoxide and reactive oxygen species (ROS) for the repair of oxidative radiation and chemotherapy damage (9). MGd is currently undergoing several clinical trials as a radiation sensitizer for brain metastases in conjunction with whole-brain radiation therapy (WBRT). It is also being actively investigated in clinical trials for the treatment of pediatric brain tumors, non-small cell lung cancers (NSCLC), lymphomas, renal cell carcinomas, and pancreatic and biliary tumors (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Motexafin gadolinium)+AND+synthesis%0D%0A)]

The ligand 4,5-diethyl-10,23-dimethyl-9,24-bis(3-hydroxypropyl)-16,-17-bis(3,hydroxypropyl)oxy-13,20,25,26,27—pentaazapentacyclo-[20.2.1.1^3,6^.1^9,11^.0^14,19^]heptacosa-3,5,8,10,12,14,16,18,20,22,24-undecaene was obtained through multiple steps of synthesis (7). First, 2-(acetoxymethyl)-5-((benzyloxy)carbonyl)-4-methyl-3-((methoxycarbonyl)ethyl)pyrrole was reacted with 3,4-diethylpyrrol to produce 2,5-bis[(5-((benzyloxy)carbonyl)-3-((methoxycarbonyl)ethyl)-4-methylpyrrol-2-yl)methyl]-3,4-diethylpyrrole in 75% yield. The product was further reduced by BH_3_ in tetrahydrofuran (THF) to produce 2,5-bis[(5-((benzyloxy)carbonyl)-3-(3-hydroxypropyl)-4-methylpyrrol-2-yl)methyl]-3,4-diethylpyrrole in 85% yield, followed by hydrogenation using 10% Pd/C to produce 2,5-bis[(3-(3-hydroxypropyl)-5-carboxyl-4-methylpyrrol-2-yl)methyl]-3,4-diethylpyrrole in near-quantitative yield. Then, the obtained compound was reacted with triethyl orthoformate and dialdehyde tripyrrane in two successive steps to produce 2,-5-bis[(5-formyl-3(3-hydroxypropyl)-4-methylpyrrol-2-yl)methyl]-3,4-diethylpyrrole in 80% yield. Finally, the product was reacted with 1,2-diamino-4,5-bis((3-hydroxypropyl)oxy)benzene to produce the ligand, which formed a complex with Gd(NO_3_)_3_ to give the chelate in 72% yield. The molecular weight of MGd was found to be 972.

MGd is commercially available (Pharmacyclics Inc, Sunnyvale, CA) and is currently undergoing a variety of clinical trials (9), including several phase III clinical trials for the treatment of brain metastasis of lung cancer in conjunction with WBRT (12-14), a phase I clinical trial for the treatment of newly diagnosed glioblastoma multiforme (15, 16), and a phase II clinical trial in patients with lymphoma and multiple myeloma (16).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Motexafin gadolinium)+AND+%22in+vitro%22)]

Nuclear magnetic relaxation dispersion (NMRD) and electron spin resonance spectroscopy at x-band were used to examine the relaxation properties for MGd in saline and in 5% human serum albumin (HSA) solution (17). The kinetic parameters were extracted by fitting the experimental NMRD curves, including the rotation correlation time (τ_R_) of 120 ps, the electronic relaxation time (τ_v_) of 46 ps, the structural water residual time (τ_m_) of ~10 ns, and the water coordination number (q) of 3.5 at 37°C. The proton relaxivity of aqueous MGd displayed much higher values than that of the conventional Gd contrast agents in the range of 0.01–50 MHz. For instance, the T_1_ relaxivity was 19.0 ± 1.5 mM^-1^s^-1^ at 20 MHz and 25°C versus 16.9 ± 1.5 mM^-1^s^-1^ at 50 MHz and 37°C. These high relaxivity values may be attributed quite simply to a combination high q and long τ_R_. In the presence of HSA, the relaxivity of MGd increased, but it was still less than the value predicted from the τ_R_ of 3 ns, which reflected a reduced q and/or longer τ_m_. Temperature-dependent measurements indicated that the relaxivity of MGd was limited by water exchange in HSA solution but not in aqueous solution. MGd was very stable and no free Gd^3+^ was detected after 7 days. The possible binding of anions like monohydrogen phosphate and dihydrogen phosphate reduced the number of axial coordination sites available for the inner-sphere water complex, as shown in the sharp decrease of the relaxivity from 18 mM^-1^s^-1^ in aqueous solution to 5.3 mM^-1^s^-1^ in 0.01 M KH_2_PO_4_/K_2_HPO_4_ buffer at 25°C and 50 MHz.

The in vitro intranuclear uptake of MGd was conducted in four well-established human glioblastoma multiforme cell lines, including T98G, U87, MO59K, and TB10 (18). A solution of 2.3 mg/ml MGd in 5% aqueous mannitol was added to the culture medium to yield a final Gd concentration of 100 μM. After 72 h incubation, the intracellular Gd was found to be 2.5 to 7.5 times greater than the extracellular Gd using inductively coupled plasma mass spectrometry (ICP-MS), and nearly 90% of intracellular Gd was located inside the nuclei.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Motexafin gadolinium) +AND++rodentia)]

Young et al. conducted a pharmacokinetic study in rats at a dose of 4 mg/kg (10). A series of blood samples were taken after a bolus injection of ^153^Gd-labeled MGd, and the concentration in blood plasma was measured by gamma (γ) counting. The half-life for the initial arterial phase was 4.2 min and 5.4 min for male and female rats, respectively. The half-life for the steady-state phase was 41.4 min and 35.4 min for male and female rats, respectively. The volume of distribution was calculated to be 0.315 L/kg for male rats and 0.265 L/kg for female rats. The 50% lethal dose (LD_50_) for rats was found to be 147 mg/kg in males and 116 mg/kg in females. The LD_50_ for mice was 118 mg/kg in males and 102 mg/kg in females.

The biodistribution was measured in healthy rats after a bolus injection of ^153^Gd-labeled MGd at a dose of 4 mg/kg (4 × 10^6^ counts/min per mg) (10). After 48 h, no detectable counts were found in the urine of male or female animals. The cumulative urine excretion after 96 h was 13.67% of the injected dose (ID) for the males and 10.53% of ID for the females. At 7 days after injection, the cumulative fecal excretion was 64% ID for the males and 77% ID for the females. Apparently, most of the fecal excretion occurred within the first 48 h with continual excretion of 1–2% per day for the remainder of the 7-day study. The liver retained the highest amount of radioactivity, and the retention decreased between 24 hours and 7 days. The decrease in radioactive counts in the liver roughly correlated with the recovery in the feces. After ~1 week, 7% ID and 3% ID remained in the carcasses of males and females, respectively. The liver-to-kidney excretion ratio was approximately 5:1, suggesting that MGd secreted into the biliary system predominantly via the liver and subsequently excreted into gastrointestinal tract. There was no retention in brain, heart, stomach, duodenum, tests, ovary, muscle, or fat. The organ biodistribution was consistent with uptake of the drug by the liver and secretion into the bile.

The subchronic toxicity study was performed in healthy rats (10). MGd was intravenously injected on Monday, Wednesday, and Friday of each week for 3 weeks at five doses of 0.0, 2.0, 5.0, 10.0, and 20.0 μmol. No difference was observed in body weight gain, clinical chemistries, and complete blood counts. No gross pathological lesions were seen in any organs or histopathological examinations. The administration of 180 μmol/kg during a 3-week period produced no biochemical or histological abnormality.

T_1_-Weighted images were acquired for healthy rats on a 1.5-T imager after injection of 17 μmol/kg MGd (10). The percent contrast enhancement increased significantly in the liver and kidney from 5 min to 2 h, and the maximum percent contrast enhancement was 81.7% and 114.9% in the liver and kidney, respectively. At a dose of ≥17 μmol/kg MGd, a slight greenish discoloration appeared on the nose tips, ear tips, and tail; this discoloration vanished in 15 min. The tumor signal enhancement was tested in rats with implanted fibrosarcomas 2.5–3.5 cm in diameter. T_1_-Weighted images were acquired before and 15 min after a bolus injection of 17 μmol/kg MGd. A 49.7% enhancement was found in the fibrosarcoma 15 min after injection, which was still detectable 28 h later. The change after a bolus injection of MGd was subsequently followed up by MRI at 0 min, 10 min, 1 h, 24 h, and 1 week. These MRI scans detected contrast enhancement of 25%, 23.3%, 23.7%, 11.2%, and 2.55%, respectively, for the 5-μmol/kg dose, and 13.15%, 11.65% 10.4%, 7.05%, and 2.6%, respectively, for the 2.5-μmol/kg dose. Similar results were found in DBA/2N mice with SMT-F neoplasmas or EMT-6 tumors (19).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Contrast enhancement efficacy was examined in rabbits with a V2 carcinoma ~2.5 cm in diameter (10, 20). The signal intensity increased dramatically up to 3.5 h after intravenous administration of 5 μmol/kg MGd. The diffusion of the agent through the tumor allowed clear distinction between the malignant tissues and the normal tissues. For rabbits with a V2 carcinoma in the liver, the study was conducted at a dose of 2.5 μmol/kg. Images were collected at 15 min, 1 h, 2 h, and 24 h. The conspicuity of the V2 carcinoma in the liver was significantly increased, and the contrast/noise ratio (C/N) was 5.5 before injection, 10.90 immediately after injection, 10.90 after 15 min, 9.94 in 1 h, and 9.46 in 2 h. The enhancement allowed for the identification of neoplasmas as small as 1 to 2 mm, which were not detectable without MGd.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Motexafin gadolinium) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Motexafin gadolinium) +AND+human)]

A phase I clinical trial was reported by Rosenthal et al. to determine the maximum tolerated dose (MTD), dose-limiting toxicity (DLT), pharmacokinetics, and biolocalization for a single-dose of MGd alone (21, 22). Thirty-eight patients (median age, 58 yrs; range, 35–77 yrs) with incurable lung cancer (n = 26), cervical cancer (n = 3), or other solid tumors (n = 9) received a total of 41 single administrations. The MTD was found to be 22.3 mg/kg with reversible acute tubular necrosis as the marker for the dose-limiting toxicity. The MGd dose was escalated from 0.6 to 29.6 mg/kg, and dose-limiting reversible renal toxicity was observed at the dose of 29.6 mg/kg. The median half-life of MGd after a single-dose administration was 7.4 h, and the maximum recommended dose for the single administration was 16.7 mg/kg. The frequently reported adverse event was transient green discoloration of skin, mucosa, feces, and urine in all of the patients that received doses ≥7.1 mg/kg. The transient increases in transaminases of grade 1 or grade 2 were observed in <5 patients. The peak appeared 48 h after injection and resolved in 7 days. MRI images demonstrated that some but not all of the tumors showed a 31% increase in signal intensities at a 4.0-mg/kg dose, but all primary and metastatic tumors exhibited a 24–113% increase in signal intensities at a dose of 5.4 mg/kg.

A combined phase Ib/II clinical trial was reported by Carde et al. to investigate the effect of 10 daily intravenous doses of MGd with concomitant WBRT (23). The MTD, DLT, pharmacokinetics, and biolocalization were determined in patients with metastases in conjunction with a 30-Gy WBRT in 10 daily fractions (23). In the phase Ib part of the trial, MGd dose was escalated from 0.3 mg/kg to 8.4 mg/kg in 39 patients. In the phase II part of the trial, 22 patients received 5 - 6.3 mg/kg. The drug-related toxicity was assessed via complete blood counts and blood chemistry, urinalysis, history, and physical examination. Patients from both groups demonstrated satisfied tolerance to the 10 once-daily treatments. The MTD was found to be 6.3 mg/kg with reversible liver toxicity. The frequency of liver toxicity did not increase with dose, but the magnitude of changes in liver functions increased with increasing dose. Overall (phases Ib and II), 12 patients (19.6%) experienced liver toxicity of any grade. and 10 patients (16%) experienced grade 3 or 4 toxicity. The most common grade 3 and grade 4 adverse events were noted in 2 patients: hepatotoxicity, hypertension, brain edema, and vomiting. The most frequent adverse events observed with repeated administration of MGd were dose-dependent, transient, greenish skin (56%) and urine (43%) discoloration, as well as scleral discoloration (18%). The other adverse events noted in at least 10% of the patients were nausea (28%), vomiting (18%), asthenia (15%), rash (13%), headache (10%), abdominal pain (10%), and pruritus (10%). On the basis of these results, a regimen of 10 once-daily doses of MGd at 5 mg/kg in conjunction with a 30-Gy WBRT in 10 daily fractions was used in phase III trials to explore the effect of MGd in conjunction with WBRT on neurocognitive function and progression in patients with brain metastases from solid tumors (12, 13, 24). No further drug-related toxicity was reported in these phase III trials.

### NIH Support

AI 28845, CA 68682

## References

1 Kessel D. (1984). Porphyrin localization: a new modality for detection and therapy of tumors. Biochem Pharmacol.
2 Ogan M.D., Revel D., Brasch R.C. (1987). Metalloporphyrin contrast enhancement of tumors in magnetic resonance imaging. A study of human carcinoma, lymphoma, and fibrosarcoma in mice. Invest Radiol.
3 Lyon R.C., Faustino P.J., Cohen J.S., Katz A., Mornex F., Colcher D., Baglin C., Koenig S.H., Hambright P. (1987). Tissue distribution and stability of metalloporphyrin MRI contrast agents. Magn Reson Med.
4 Chen C.W., Cohen J.S., Myers C.E., Sohn M. (1984). Paramagnetic metalloporphyrins as potential contrast agents in NMR imaging. FEBS Lett.
5 Lauffer R.B., Brady T.J., Brown R.D., Baglin C., Koenig S.H. (1986). 1/T1 NMRD profiles of solutions of Mn2+ and Gd3+ protein-chelate conjugates. Magn Reson Med.
6 Sessler J.L., Murai T., Hemmi G. (1989). A water-stable gadolinium (III) complex derived from a new pentadentate "expanded porphyrin" ligand. Inorg. Chem.
7 Sessler J.L., Mody T.D., Hemmi G.W., Lynch V. (1993). Synthesis and structural characterization of lanthanide(III) texaphyrins. Inorg. Chem.
8 Sessler, J.L., G. Hemmi, T.D. Mody, T. Murai, A. Burrell, and S.w. Young, Texaphyrins: synthesis and applications. Acc. Chem. Res., 1994. 27(43-50): p. 43.
9 Richards G.M., Mehta M.P. (2007). Motexafin gadolinium in the treatment of brain metastases. Expert Opin Pharmacother.
10 Young S.W., Sidhu M.K., Qing F., Muller H.H., Neuder M., Zanassi G., Mody T.D., Hemmi G., Dow W., Mutch J.D., et al. (1994). Preclinical evaluation of gadolinium (III) texaphyrin complex. A new paramagnetic contrast agent for magnetic resonance imaging. Invest Radiol.
11 Magda D., Miller R.A. (2006). Motexafin gadolinium: a novel redox active drug for cancer therapy. Semin Cancer Biol.
12 Mehta M.P., Rodrigus P., Terhaard C.H., Rao A., Suh J., Roa W., Souhami L., Bezjak A., Leibenhaut M., Komaki R., Schultz C., Timmerman R., Curran W., Smith J., Phan S.C., Miller R.A., Renschler M.F. (2003). Survival and neurologic outcomes in a randomized trial of motexafin gadolinium and whole-brain radiation therapy in brain metastases. J Clin Oncol.
13 Meyers C.A., Smith J.A., Bezjak A., Mehta M.P., Liebmann J., Illidge T., Kunkler I., Caudrelier J.M., Eisenberg P.D., Meerwaldt J., Siemers R., Carrie C., Gaspar L.E., Curran W., Phan S.C., Miller R.A., Renschler M.F. (2004). Neurocognitive function and progression in patients with brain metastases treated with whole-brain radiation and motexafin gadolinium: results of a randomized phase III trial. J Clin Oncol.
14 Mehta M.P., Shapiro W.R., Glantz M.J., Patchell R.A., Weitzner M.A., Meyers C.A., Schultz C.J., Roa W.H., Leibenhaut M., Ford J., Curran W., Phan S., Smith J.A., Miller R.A., Renschler M.F. (2002). Lead-in phase to randomized trial of motexafin gadolinium and whole-brain radiation for patients with brain metastases: centralized assessment of magnetic resonance imaging, neurocognitive, and neurologic end points. J Clin Oncol.
15 Khuntia D., Mehta M. (2004). Motexafin gadolinium: a clinical review of a novel radioenhancer for brain tumors. Expert Rev Anticancer Ther.
16 (2004). Motexafin gadolinium: gadolinium (III) texaphyrin, gadolinium texaphyrin, Gd-Tex, GdT2B2, PCI 0120. Drugs R D.
17 Geraldes C.F., Sherry A.D., Vallet P., Maton F., Muller R.N., Mody T.D., Hemmi G., Sessler J.L. (1995). Nuclear magnetic relaxation dispersion studies of water-soluble gadolinium(III)-texaphyrin complexes. J Magn Reson Imaging.
18 De Stasio G., Rajesh D., Ford J.M., Daniels M.J., Erhardt R.J., Frazer B.H., Tyliszczak T., Gilles M.K., Conhaim R.L., Howard S.P., Fowler J.F., Esteve F., Mehta M.P. (2006). Motexafin-gadolinium taken up in vitro by at least 90% of glioblastoma cell nuclei. Clin Cancer Res.
19 Young S.W., Qing F., Harriman A., Sessler J.L., Dow W.C., Mody T.D., Hemmi G.W., Hao Y., Miller R.A. (1996). Gadolinium(III) texaphyrin: a tumor selective radiation sensitizer that is detectable by MRI. Proc Natl Acad Sci U S A.
20 Sessler, J.L., T.D. Mody, V. Lynch, S.W. Young, and R.A. Miller, Gadolinium(III) texaphyrin: a novel MRI contrast agent. J. Am. Chem. Soc., 1993. 115(10368-9): p. 10368.
21 Rosenthal D.I., Nurenberg P., Becerra C.R., Frenkel E.P., Carbone D.P., Lum B.L., Miller R., Engel J., Young S., Miles D., Renschler M.F. (1999). A phase I single-dose trial of gadolinium texaphyrin (Gd-Tex), a tumor selective radiation sensitizer detectable by magnetic resonance imaging. Clin Cancer Res.
22 Rosenthal D.I., Becerra C.R., Toto R.D., Carbone D.P., Frenkel E.P. (2000). Reversible renal toxicity resulting from high single doses of the new radiosensitizer gadolinium texaphyrin. Am J Clin Oncol.
23 Carde P., Timmerman R., Mehta M.P., Koprowski C.D., Ford J., Tishler R.B., Miles D., Miller R.A., Renschler M.F. (2001). Multicenter phase Ib/II trial of the radiation enhancer motexafin gadolinium in patients with brain metastases. J Clin Oncol.
24 Mehta M.P., Suh J.H. (2004). Novel radiosensitizers for tumors of the central nervous system. Curr Opin Investig Drugs.